# Cy5.5-Polyethylene glycol-CGS25966 inhibitor of matrix metalloproteinases

Chemical name: | Cy5.5-Polyethylene glycol-CGS25966 inhibitor of matrix metalloproteinases
Abbreviated name: | Cy5.5-AF489
Synonym: | Cy5.5-PEG-CGS25988, CGS-Cy5.5
Agent category: | Compound
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). There are four members of endogenous tissue inhibitors of metalloproteinases (TIMP1-4), which regulate the activity of MMPs and lead to the inhibition of tumor growth and metastasis (9, 10). CGS25966 is a broad-spectrum, small-molecule inhibitor of MMPs (11). Faust et al. (11) inserted a polyethylene glycol (PEG) linker with an amino functional group for conjugation with the near-infrared (NIR) fluorescence dye Cy5.5 to form Cy5.5-PEG-CGS25966 (CY5.5-AF489). Waschkau et al. (12) evaluated Cy5.5-AF489 for use with in vivo NIR fluorescence imaging of tumors with high or low MMP-2/MMP-9 expression in nude mice.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D), TIMP (http://www.ncbi.nlm.nih.gov/books?term=TIMP%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (TIMP-2 (http://www.ncbi.nlm.nih.gov/gene/7077), MMP-2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP-8 (http://www.ncbi.nlm.nih.gov/gene/4317), MMP-9 (http://www.ncbi.nlm.nih.gov/gene/4318), MMP-13 (http://www.ncbi.nlm.nih.gov/gene/4322))
- Articles in Online Mendelian Inheritance in Man (OMIM) (TIMP-2 (http://omim.org/entry/188825), MMP-2 (http://omim.org/entry/120360), MMP-8 (http://omim.org/entry/120355), MMP-9 (http://omim.org/entry/120361), MMP-13 (http://omim.org/entry/600108))
- Clinical trials (TIMP (http://www.clinicaltrials.gov/ct2/results?term=TIMP), MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (TIMP (http://google2.fda.gov/search?q=TIMP&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489)]

A solution of Cy5.5-N-hydroxysuccinimide ester (0.9 µmol) and the amino derivative ((R)-2-(N-(4-(2-(2-(2-(2-aminoethoxy)ethoxy)ethoxy)ethoxy)benzyl)-4-methoxyphenylsulfon-amido)-N-hydroxy-3-methylbutanamide) (1.7 µmol) was incubated for 2 h at 25°C (12). Cy5.5-AF489 was purified with high-performance liquid chromatography, with 43% yield and >97% purity. Mass spectroscopy analysis confirmed conjugation of Cy5.5 to the amino derivative. Cy5.5-AF489 exhibited a molecular weight of 1.45 kDa. Fluorescence absorption maximum of Cy5.5-AF489 was 678 nm, with an excitation coefficient of 250,000 M−^1^cm−^1^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489%20and%20in%20vitro)]

Using in vitro enzyme activity inhibition assays, Cy5.5-AF489 exhibited IC_50_ values of 1.5 ± 0.6 nM, 1.8 ± 0.2 nM, 2.1 ± 0.1 nM, and 1.7 ± 0.3 nM for MMP-2, MMP-8, MMP-9, and MMP-13 (12), respectively. In vitro cellular fluorescence MMP-binding assays of Cy5.5-AF489 were performed with tumor sections of human rhabdomyosarcoma A-673 (high MMP-2/MMP-9 expression), fibrosarcoma HT-1080 (weak MMP-2/MMP-9 expression), and mammary carcinoma BT-20 (low MMP-2/MMP-9 expression). High fluorescence intensity rank order (Cy5.5-AF489 binding) was A-673 > HT-1080 > BT-20. Furthermore, Cy5.5-AF489 fluorescence was colocalized with MMP-2 and MMP-9 in the A-673 tumor sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489%20and%20rodentia)]

Waschkau et al. (12) performed ex vivo optical imaging studies of Cy5.5-AF489 (2 nmol/mouse) in nude mice bearing A-673 tumors at 6 h (n = 12), 24 h (n = 12), and 72 h (n = 20). High NIR fluorescence levels were observed for the tumor (282.4 ± 56.9 arbitrary units, AU) and kidneys (197.1 ± 14.5 AU), followed by the lungs (150.5 ± 39.5 AU) and liver (113.7 ± 25.5) at 6 h after injection. Low fluorescence signal was observed in the spleen, muscle, heart, and brain. NIR fluorescence intensity in the tumor and normal tissues was reduced by 50% at 24 h and was mostly eliminated by 72 h. The level of Cy5.5-AF489 remained at 20% of injected dose in the blood at 6 h and <10% at 24 h.

Whole-body fluorescence reflectance imaging was performed for up to 72 h in mice bearing A-673, HT-1080, MDA-MB 231, or BT-20 xenografts after injection of Cy5.5-AF489 (2 nmol/mouse) (12). A rapid and clear visualization of the tumors was observed at 30–45 min, and visualization remained consistent for ~5 h before declining to the fluorescence levels of the abdomen and muscle by 72 h. A-673 tumors (727.7 ± 44.2 AU) exhibited higher signal than HT-1080 (569.9 ± 14.1 AU), MDA-MB-231 (519.9 ± 15.2 AU), and BT-20 (468.3 ± 37.3 AU) tumors. Fluorescence intensities were 320–350 AU for the abdomen and muscle at 6 h. The maximal tumor/muscle ratios were 2.3, 1.8, 1.6, and 1.6 for A-673, HT-1080, MDA-MB 231, and BT-20 tumors, respectively. NIR fluorescence signal in A-673 tumors was inhibited by 34% after pretreatment with the MMP inhibitor CGS27023A (200 nmol, 15 min) (P < 0.05). There was a significant correlation between NIR fluorescence intensities and MMP-2/MMP-9 levels in the four tumors (P < 0.001).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AF489%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Baker A.H., Edwards D.R., Murphy G. (2002). Metalloproteinase inhibitors: biological actions and therapeutic opportunities. J Cell Sci.
10 Jiang Y., Goldberg I.D., Shi Y.E. (2002). Complex roles of tissue inhibitors of metalloproteinases in cancer. Oncogene.
11 Faust A., Waschkau B., Waldeck J., Holtke C., Breyholz H.J., Wagner S., Kopka K., Schober O., Heindel W., Schafers M., Bremer C. (2009). Synthesis and evaluation of a novel hydroxamate based fluorescent photoprobe for imaging of matrix metalloproteinases. Bioconjug Chem.
12 Waschkau B., Faust A., Schafers M., Bremer C. (2013). Performance of a new fluorescence-labeled MMP inhibitor to image tumor MMP activity in vivo in comparison to an MMP-activatable probe. Contrast Media Mol Imaging.